# ^99m^Tc-Hydrazinonicotinamide-interleukin-8

Chemical name: | ^99m^Tc-Hydrazinonicotinamide-interleukin-8
Abbreviated name: | ^99m^Tc-HYNIC-IL-8, ^99m^Tc-IL-8
Synonym:
Agent Category: | Polypeptide
Target: | IL-8 receptors (CXC1 and CXC2)
Target Category: | Receptor binding
Method of detection: | SPECT, planar
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Non-primate non-rodent mammals; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=15488984), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=28610153) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3576) for more information about IL-8.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-Interleukin-8%20or%2099mTc-IL-8)]

Interleukin-8 (IL-8) has a molecular mass of 8.5 kDa and is an inflammatory chemokine secreted by many cell types (1). It activates neutrophils and monocytes and also serves as a chemoattractant. Therefore, IL-8 plays an important role in cell recruitment during acute inflammation and infection. Two types (CXC1 and CXC2) of high-affinity (0.3–4 nM) IL-8 receptors (IL-8Rs) have been identified abundantly on the cell surface of neutrophils (2).

^99m^Tc-IL-2 has been developed as a single-photon emission computed tomography (SPECT) tracer for imaging activated immune cells in tumors and pathological tissues. Therefore, it is feasible to label this polypeptide for imaging studies. The ready availability and low cost of ^99m^Tc led to the development of ^99m^Tc-IL-8 for studying activated leukocytes in inflamed and infective tissues (3-8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-Interleukin-8%20or%2099mTc-IL-8%29%20and%20synthesis)]

Rennen et al. (7) reported a two-step synthesis of ^99m^Tc-IL-8 using the bifunctional chelating agent succinimidyl-hydrazinonicotinic acid (S-HYNIC), a ligand with two active sites: one for protein conjugation with the amino groups on lysine residues of IL-8, and the other for coordination of ^99m^Tc. IL-8 was incubated for 10 min at room temperature with three-fold molar excess of HYNIC. The reaction was stopped by addition of an excess of glycine. After purification, 500–1,000 MBq (13.5–27.0 mCi) of ^99m^TcO_4_^-^ in saline (containing tricine and SnSO_4_) was added to 5–20 µg of IL-8–HYNIC. The mixture was incubated at 70°C for 30 min. Radiochemical purity was >95% after column chromatography with a specific activity of 24 GBq/μmol (0.65 Ci/μmol). The labeling efficiency was 20%. Addition of nicotinic acid to the co-ligand system improved the specific activity to 425 GBq/μmol (11.5 Ci/μmol) (3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-Interleukin-8%20or%2099mTc-IL-8%29%20and%20in%20vitro)]

Rennen et al. (7) reported that the receptor-binding capacity of ^99m^Tc-IL-8 was largely preserved after radiolabeling. The receptor-binding fraction for conditions representing infinite IL-8 receptor excess was ~65%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-Interleukin-8%20or%2099mTc-IL-8%29%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-Interleukin-8%20or%2099mTc-IL-8%29%20and%20rabbit)]

Rennen et al. (5) performed biodistribution studies of ^99m^Tc-HYNIC-IL-8 in 10 female rabbits with Escherichia coli infection in the left thigh muscle. Immediately after injection of ^99m^Tc-HYNIC-IL-8 (13 pmol/kg ), a transient 54% reduction of peripheral leukocytes was observed at 30 min after injection. The blood clearance pattern exhibited a two-phase model with a half-life (t_1/2_α) of 4.2 min during the distribution phase and a half-life (t_1/2_ß) of 5.1 h during the elimination phase. The abscesses were clearly delineated on the SPECT images recorded from 1 h onward. ^99m^Tc-HYNIC-IL-8 rapidly accumulated at the site of infection. Quantitative analysis of the SPECT images indicated that the abscess/background ratios improved with time up to 21.8 ± 1.0 at 8 h after injection. High kidney uptake was observed immediately after injection and remained high during the 8-h imaging duration. In addition, high radioactivity was found in the bladder, liver, and lungs. The control agent, ^99m^Tc-HYNIC-lysozyme, showed a similar kidney uptake pattern but failed to accumulate significantly at the site of infection. Abscess/background ratios did not exceed 2.7. Except for the kidneys and spleen, the highest accumulation of radioactivity was found in the abscess: 0.33 ± 0.06% injected dose/g (% ID/g) versus 0.025 ± 0.003% ID/g for ^99m^Tc-HYNIC-lysozyme (P = 0.0001). Total accumulation in the infected tissue was 4.9 ± 0.7% ID/g versus 0.44 ± 0.05% ID/g for ^99m^Tc-HYNIC-lysozyme (P = 0.0001), which indicated preferential retention of ^99m^Tc-HYNIC-IL-8 in infected tissue. Abscess/muscle ratio reached a value of 127 ± 23 at 8 h after injection versus 6.7 ± 1.1 for ^99m^Tc-HYNIC-lysozyme (P < 0.001). The abscess-to-blood ratio was 11.9 ± 2.2 at 8 h after injection compared with 0.24 ± 0.03 for ^99m^Tc-HYNIC-lysozyme (P = 0.0001). Kidney retention of ^99m^Tc-HYNIC-IL-8 was high with 28 ± 1% ID/g at 8 h after injection (35 ± 1% ID/g for ^99m^Tc-HYNIC-lysozyme).

Rennen et al. (6) compared ^99m^Tc-HYNIC-IL-8 accumulation in turpentine-induced inflammation in neutropenic rabbits (n = 5) with accumulation in turpentine-induced inflammation in normal rabbits (n = 4). The abscess accumulation in immunocompetent rabbits (0.41 ± 0.05) was 10 times higher than that in neutropenic rabbits (0.038 ± 0.014), which demonstrated specificity of the target accumulation of ^99m^Tc-HYNIC-IL-8. Abscess/muscle ratios were also 10 times higher (110 ± 10 versus 10 ± 5). Lung and spleen accumulation in normal rabbits was 3 times higher than that in neutropenic rabbits. The blood clearance of the radiolabel in neutropenic rabbits was similar to that in normal rabbits. In circulation, 70% of ^99m^Tc-HYNIC-IL-8 was found in the plasma fraction. Less than one-third was associated with red blood cells, and only a very low percentage (<2.5%) was associated with white blood cells. Image analysis revealed a gradually increasing abscess accumulation of ^99m^Tc-HYNIC-IL-8 over time up to >15% ID/g. The highest increase in accumulation in the abscess was observed 2 h after injection, when >85% of ^99m^Tc-HYNIC-IL-8 was cleared from the blood, which suggested specific neutrophil-mediated accumulation of ^99m^Tc-HYNIC-IL-8 in the abscess. Furthermore, region-of-interest analysis revealed that gradual accumulation of ^99m^Tc-HYNIC-IL-8 in the abscess was accompanied by a simultaneous clearance of radioactivity from the lungs, which suggested that neutrophil-associated ^99m^Tc-HYNIC-IL-8 was initially trapped in the lungs and migrated to the abscess at later time points.

Further experiments in rabbits revealed high accumulation of ^99m^Tc-HYNIC-IL-8 in experimental models of pulmonary infections (8), colitis (9), and osteomyelitis (10).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-Interleukin-8%20or%2099mTc-IL-8%29%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-IL-8%20and%20human)]

Bleeker-Rovers et al. performed ^99m^Tc-HYNIC-IL-8 scintigraphy in 20 patients (13 men and 7 women; age range 21–76 years) with various suspected localized infection (11). There was accumulation of ^99m^Tc-HYNIC-IL-8 in 10 of 12 with confirmed infection at 4 h after injection. Two patients were false-negative. No focal accumulation was detected in 8 patients with noninfectious disorders. The blood clearance pattern exhibited a two-phase model with a distribution t_1/2_α of 7.5 min and an elimination half-life t_1/2_ß of 4.6 h. The organ with the highest accumulation was the kidney, followed by the spleen, urinary bladder, and liver. The effective dose was estimated to be 6.8 μSv/MBq (25 mrem/mCi).

## References

1 Patel L., Charlton S.J., Chambers J.K., Macphee C.H. (2001). Expression and functional analysis of chemokine receptors in human peripheral blood leukocyte populations. Cytokine.
2 Lee J., Horuk R., Rice G.C., Bennett G.L., Camerato T., Wood W.I. (1992). Characterization of two high affinity human interleukin-8 receptors. J Biol Chem.
3 Rennen H.J., van Eerd J.E., Oyen W.J., Corstens F.H., Edwards D.S., Boerman O.C. (2002). Effects of coligand variation on the in vivo characteristics of Tc-99m-labeled interleukin-8 in detection of infection. Bioconjug Chem.
4 Rennen H.J., Frielink C., Brandt E., Zaat S.A., Boerman O.C., Oyen W.J., Corstens F.H. (2004). Relationship between neutrophil-binding affinity and suitability for infection imaging: comparison of (99m)Tc-labeled NAP-2 (CXCL-7) and 3 C-terminally truncated isoforms. J Nucl Med.
5 Rennen H.J., Boerman O.C., Oyen W.J., van der Meer J.W., Corstens F.H. (2001). Specific and rapid scintigraphic detection of infection with 99mTc-labeled interleukin-8. J Nucl Med.
6 Rennen H.J., Boerman O.C., Oyen W.J., Corstens F.H. (2003). Kinetics of 99mTc-labeled interleukin-8 in experimental inflammation and infection. J Nucl Med.
7 Rennen H.J., Boerman O.C., Koenders E.B., Oyen W.J., Corstens F.H. (2000). Labeling proteins with Tc-99m via hydrazinonicotinamide (HYNIC): optimization of the conjugation reaction. Nucl Med Biol.
8 Rennen H.J., Bleeker-Rovers C.P., van Eerd J.E., Frielink C., Oyen W.J., Corstens F.H., Boerman O.C. (2004). 99mTc-labeled interleukin-8 for scintigraphic detection of pulmonary infections. Chest.
9 Gratz S., Rennen H.J., Boerman O.C., Oyen W.J., Corstens F.H. (2001). Rapid imaging of experimental colitis with (99m)Tc-interleukin-8 in rabbits. J Nucl Med.
10 Gratz S., Rennen H.J., Boerman O.C., Oyen W.J., Burma P., Corstens F.H. (2001). (99m)Tc-interleukin-8 for imaging acute osteomyelitis. J Nucl Med.
11 Bleeker-Rovers C.P., Rennen H.J., Boerman O.C., Wymenga A.B., Visser E.P., Bakker J.H., van der Meer J.W., Corstens F.H., Oyen W.J. (2007). 99mTc-Labeled Interleukin 8 for the Scintigraphic Detection of Infection and Inflammation: First Clinical Evaluation. J Nucl Med.